# Fibroblast activation protein α–specific, near-infrared peptide probe (KGPGPNQC) linked to Cy5.5 and a quencher dye, QSY21

Chemical name: | Fibroblast activation protein α–specific, near-infrared peptide probe (KGPGPNQC) linked to Cy5.5 and a quencher dye, QSY21 | [image]
Abbreviated name: | ANP_FAP_ | [image]
Synonym: | | [image]
Agent Category: | Peptide | [image]
Target: | Fibroblast activation protein-α | [image]
Target Category: | Enzyme | [image]
Method of detection: | Near-infrared (NIFR) imaging; optical imaging | [image]
Source of signal / contrast: | Cy5.5 | [image]
Activation: | Yes | [image]
Studies: | - In vitro; - Rodents | Structure of ANP_FAP_

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=fibroblast%20activation%20protein%20review&cmd=DetailsSearch)]

The fibroblast activation protein α (FAPα; also known as seprase) is a tumor stromal fibroblast cell-surface dipeptidyl peptidase IV (DPPIV) serine protease that is expressed in various pathologies such as cancers (colon-rectal, pancreas, lung, ovarian, etc.), arthritis, fibrosis, and inflammation, but not in normal tissues (1). Although the exact function of FAPα in the development of the different diseases is not clear, it is believed to participate in the progression and metastasis of cancer, angiogenesis, and the suppression of the antitumor response of the immune system (1). Because of its role in the ontogeny of various pathological conditions, FAPα is considered an excellent target for the detection and treatment of different diseases, particularly cancer (2). A small molecule inhibitor of FAPα has been evaluated in a phase II clinical trial for the treatment of metastatic colorectal cancer (3). Therefore, probes that can be used with noninvasive imaging can be of much value for the early detection of cancer, to screen for patients who would benefit most from an anti-FAPα therapy, and to monitor patients for treatment response (4).

Targeted, activatable, near-infrared (NIR) fluorescent probes (ANP_FAP_) based on fluorescence resonance energy transfer (FRET), that target proteases such as matrix metalloproteinases (MMP) (5), cysteine proteases (6), and caspase (7) have been successfully used to detect cancerous tumors. However, no such probe that targets the FAPα is available (4). Li et al. developed a FRET probe that was selectively activated by FAPα, and showed that it was suitable for the in vivo detection of tumors that express activation protein in mice (4). The probe consists of the NIR dye Cy5.5, which is linked to QSY21, a quencher dye, through a peptide (ANP; sequence KGPGPNQC) that specifically binds to and is a substrate for the FAPα.

### Related Resource Links

Related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=FRET+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Clinical trials (http://clinicaltrials.gov/ct2/results?term=fibroblast+activation+protein&Search=Search) related to FAPα

FAPα in Gene database (http://www.ncbi.nlm.nih.gov/gene/2191) (Gene ID: 2191)

FAPα (http://omim.org/entry/600403) in Online Mendalian Inheritance in man database (OMIM)

Protein and mRNA (http://www.ncbi.nlm.nih.gov/nuccore/NM_004460.2) sequences of human FAPα (seprase)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Fibroblast%20activation%20protein%20probe%20synthesis&cmd=DetailsSearch)]

The synthesis of ANP_FAP_ peptide has been described by Li et al. (4). The substrate peptide was synthesized on an automatic peptide synthesizer. The final product was purified with reverse-phase high-performance liquid chromatography (RP-HPLC) and characterized with matrix-assisted laser desorption-ionization time-of-flight mass spectrometry (MALDI-TOF-MS). The purified peptide was then conjugated with Cy5.5, and the NIR dye-labeled ANP was purified with RP-HPLC. The Cy5.5-peptide was characterized with MALDI-TOF-MS before use for the next step. The Cy5.5-peptide was then conjugated with QSY21 to obtain ANP_FAP_, the activatable NIR probe. The final preparation of ANP_FAP_ was purified with RP-HPLC and characterized with MALDI-TOF-MS. The final yield of ANP_FAP_ was reported to be ~26% and had a purity of >95%.

A fluorescence spectrum analysis of Cy5.5-labeled ANP and ANP_FAP_ showed that the quenching efficiency of QSY21 in the probe was 94% (4).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Fibroblast%20activation%20protein%20probe%20In%20Vitro%20Studies&cmd=DetailsSearch)]

The specificity of ANP_FAP_ for FAPα was established by incubating 10 μM of the probe with 1 μg/mL FAPα, 1 μg/mL DPPIV, and 1 μg/mL MMP, respectively, for 1 h at 37°C (4). At the end of incubation, only the ANP_FAP_/FAPα reaction showed a 12-fold increase in fluorescence emission intensity compared with controls (ANP_FAP_ incubated without FAPα under the same in vitro conditions as the test samples), and the fluorescence emission spectrum of the ANP_FAP_/FAPα reaction corresponded to that of Cy5.5. No increase in fluorescence emission was observed with either DPPIV or MMP. This indicated that the ANP_FAP_ probe was cleaved only by FAPα, and the release of QSY21 from the FRET pair resulted in the generation of fluorescence by Cy5.5. Incubation of ANP_FAP_ with increasing concentrations of FAPα (ranging from 0.25 μg/mL to 1.0 μg/mL) for 1 h at 37°C showed that the increase of fluorescence in the reaction mixture corresponded well with the amount of FAPα present in the reaction mixture (4).

The expression of FAPα in U87MG cells (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=HTB-14&Template=cellBiology) (human glioblastoma cells that express FAPα) and C6 cells (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CCL-107&Template=cellBiology) (rat fibroblasts that do not express FAPα), which were used to generate tumors in mice, was confirmed with Western blot analysis (4). An anti-FAP monoclonal antibody (Ab) was used as the primary Ab for the blots, and the protein bands were visualized with an anti-rabbit horseradish peroxidase–conjugated secondary Ab. From the blots it was evident that only the U87MG cells expressed high levels of FAPα.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Fibroblast%20activation%20protein%20probe%20rodentia&cmd=DetailsSearch)]

Mice bearing C6 cell tumors (controls) or U87MG cell tumors (n = 5 animals/group) were injected with 1 nmol ANP_FAP_ through the tail vein, and whole-body fluorescence images of the rodents were acquired at time points ranging from 0.5 h to 4 h postinjection (p.i.), with the use of a Cy5.5 filter (background 580–610 nm; excitation 615–665 nm and emission 695–770 nm) as described by Li et al. (4). For comparison, all of the fluorescence emission data were normalized to photons per second per centimeter squared per steradian (http://www.princeton.edu/~achaney/tmve/wiki100k/docs/Steradian.html) (p/s/cm^2^/sr). In contrast to the C6 cell tumors, strong fluorescent signals were obtained from the U87MG cell tumors (P < 0.05) at 0.5 h p.i. The intensity of the fluorescence signals from the U87MG lesions peaked at 2 h p.i. and remained constant thereafter. No such increase in fluorescence signal intensity was observed with the C6 cell tumors. The tumor/normal tissue fluorescence ratios (T/N ratio) of the U87MG lesions increased from 2.22 ± 0.40 at 0.5 h p.i. to 4.63 ± 0.73 at 4 h p.i., indicating there was an accumulation of the Cy5.5 probe in the tumors. The T/N ratio of the C6 cell tumors remained constant during the same time period. Although no blocking studies were reported, the investigators concluded that ANP_FAP_ exhibited a high in vivo specificity to target FAPα expressed on the U87MG cell lesions in rodents.

At the end of the imaging session at 4 h p.i., the rodents were euthanized, and all organs of interest, including the tumors, were retrieved from the animals for ex vivo imaging (4). The U87MG cell tumors had a significantly higher fluorescence signal (P < 0.05) compared with the C6 cell lesions as observed earlier during the in vivo studies. The high fluorescence signal generated in the stomachs of mice in both groups was attributed to the autofluorescence of mouse chow present in these organs. All other organs from the two groups of animals produced comparable low fluorescence signals. The T/N ratio of the U87MG cell tumors was significantly higher (P < 0.05) than that of the C6 cell tumors (~30 versus ~9).

From these studies, the investigators concluded that ANP_FAP_ was a suitable probe to detect tumors that express FAPα in rodents (4).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Fibroblast%20activation%20protein%20probe%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Fibroblast%20activation%20protein%20probe%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Fibroblast%20activation%20protein%20probe%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

Supported in part by grant 5R01 CA119053 from the National Cancer Institute of the National Institutes of Health.

## References

1 Kelly T., Huang Y., Simms A.E., Mazur A. (2012). Fibroblast activation protein-alpha: a key modulator of the microenvironment in multiple pathologies. Int Rev Cell Mol Biol.
2 Lo P.C., Chen J., Stefflova K., Warren M.S., Navab R., Bandarchi B., Mullins S., Tsao M., Cheng J.D., Zheng G. (2009). Photodynamic molecular beacon triggered by fibroblast activation protein on cancer-associated fibroblasts for diagnosis and treatment of epithelial cancers. J Med Chem.
3 Narra K., Mullins S.R., Lee H.O., Strzemkowski-Brun B., Magalong K., Christiansen V.J., McKee P.A., Egleston B., Cohen S.J., Weiner L.M., Meropol N.J., Cheng J.D. (2007). Phase II trial of single agent Val-boroPro (Talabostat) inhibiting Fibroblast Activation Protein in patients with metastatic colorectal cancer. Cancer Biol Ther.
4 Li J., Chen K., Liu H., Cheng K., Yang M., Zhang J., Cheng J.D., Zhang Y., Cheng Z. (2012). Activatable near-infrared fluorescent probe for in vivo imaging of fibroblast activation protein-alpha. Bioconjug Chem.
5 Roy R., Zurakowski D., Pories S., Moss M.L., Moses M.A. (2011). Potential of fluorescent metalloproteinase substrates for cancer detection. Clin Biochem.
6 Abd-Elgaliel W.R., Cruz-Monserrate Z., Logsdon C.D., Tung C.H. (2011). Molecular imaging of Cathepsin E-positive tumors in mice using a novel protease-activatable fluorescent probe. Mol Biosyst.
7 Barnett E.M., Zhang X., Maxwell D., Chang Q., Piwnica-Worms D. (2009). Single-cell imaging of retinal ganglion cell apoptosis with a cell-penetrating, activatable peptide probe in an in vivo glaucoma model. Proc Natl Acad Sci U S A.